# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-benzyl-ChL6-superparamagnetic iron oxide nanoparticles

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-benzyl-ChL6-superparamagnetic iron oxide nanoparticles
Abbreviated name: | ^111^In-DOTA-Bz-ChL6-SPIO
Synonym:
Agent Category: | Antibody
Target: | Integral membrane glycoprotein
Target Category: | Antibody-antigen binding
Method of detection: | Magnetic resonance imaging (MRI), SPECT gamma planar
Source of signal/contrast: | Iron oxide, ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=ChL6%20SPIO)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the nuclear density (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

The superparamagnetic iron oxide (SPIO) structure is composed of ferric iron (Fe^3+^) and ferrous iron (Fe^2+^). The iron oxide nanoparticles are coated with a layer of dextran or other polysaccharide. These nanoparticles have large combined magnetic moments or spins, which are randomly rotated in the absence of an applied magnetic field. SPIO is used mainly as a T2 contrast agent in MRI, though it can shorten both T1 and T2/T2* relaxation processes. SPIO nanoparticle uptake into the reticuloendothelial system is by endocytosis or phagocytosis. SPIO nanoparticles are also taken up by phagocytic cells such as monocytes, macrophages, and oligodendroglial cells. A variety of cells can also be labeled with these particles for cell trafficking and tumor-specific imaging studies (1). Nanoparticles have been used to deliver heat selectively at tumor sites with external alternating magnetic fields (2, 3).

ChL6 is a chimeric mouse-human IgG_1_ monoclonal antibody (mAb) against an integral membrane glycoprotein expressed in non-small cell lung, colon, and breast cancers (4). Natarajan et al. (5) reported the development of a multimodality imaging agent, ^111^In-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-benzyl-ChL6-SPIO (^111^In-DOTA-Bz-ChL6-SPIO), for imaging tumors; single-photon emission computed tomography made use of the ^111^In component of the agent, and MRI made use of the SPIO component.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6+SPIO+synthesis)]

The synthesis of ^111^In-DOTA-Bz-ChL6-SPIO nanoparticles was described by Natarajan et al. (5). DOTA-Bz-ChL6 was prepared by incubation of 0.15 mM ChL6 mAb and 2.0 mM DOTA-Bz-SCN for 2 h at 37°C. DOTA-Bz-ChL6 was purified with column chromatography and then incubated with ^111^InCl_3_ for 30 min at 37°C. Purified ^111^In-DOTA-Bz-ChL6 was conjugated to carboxyl groups of dextran/polyethylene glycol-coated SPIO nanoparticles. Three different sizes of nanoparticles were used (20, 30, and 110 nm in diameter). ^111^In-DOTA-Bz-ChL6-SPIO exhibited specific activities of 0.22 – 0.37 MBq/mg (6–10 µCi/mg) nanoparticles with yields of 26% to 35%. There were 6–10 ^111^In-DOTA-ChL6 molecules per nanoparticle. The preparations were >90% monomeric.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6%20SPIO+in+vitro)]

Radioimmunoreactivity of ^111^In-DOTA-Bz-ChL6-SPIO nanoparticles was determined with HTB 3477 human breast cancer cells to be 57% to 79% (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6%20SPIO+rodentia)]

Natarajan et al. (5) performed biodistribution studies in athymic mice bearing human breast cancer (HBT 3477) xenografts. ^111^In-DOTA-Bz-ChL6-SPIO nanoparticles (2.2 mg) were injected into the mice. Blood and various tissues were analyzed at 4, 24, and 48 h. Specific activities of the doses were 0.74–0.93 MBq/2.2mg (20–25 µCi/2.2 mg) and 6–11 µg of mAb/2.2 mg of nanoparticles. Mean tumor uptakes (% injected dose (ID)/g) of each type of ^111^In-DOTA-Bz-ChL6-SPIO nanoparticle (20 nm, 30 nm, and 100 nm in diameter) at 48 h were 9.00 ± 0.8, 3.0 ± 0.3, and 4.5 ± 0.8, respectively. The 100-nm SPIO nanoparticles had the fastest body clearance time, and the 20-nm SPIO nanoparticles had the slowest body clearance. Tissues with the highest accumulation were liver (16–32% ID/g), kidney (7–15% ID/g), spleen (8–17% ID/g), lymph nodes (5–6% ID/g), and lung (2–4% ID/g) for the three sizes of SPIO. Control ^111^In-DOTA-Bz-SPIO (20 nm) and ^111^In-DOTA-Bz-IgG-SPIO nanoparticles exhibited <0.5% ID/g accumulation in the tumor. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6%20SPIO+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6%20SPIO+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ChL6%20SPIO+human)]

No publication is currently available.

## NIH Support

PO1 CA47829

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Ito A., Honda H., Kobayashi T. (2006). Cancer immunotherapy based on intracellular hyperthermia using magnetite nanoparticles: a novel concept of "heat-controlled necrosis" with heat shock protein expression. Cancer Immunol Immunother.
3 DeNardo S.J., DeNardo G.L., Natarajan A., Miers L.A., Foreman A.R., Gruettner C., Adamson G.N., Ivkov R. (2007). Thermal dosimetry predictive of efficacy of 111In-ChL6 nanoparticle AMF--induced thermoablative therapy for human breast cancer in mice. J Nucl Med.
4 Goodman G.E., Hellstrom I., Yelton D.E., Murray J.L., O'Hara S., Meaker E., Zeigler L., Palazollo P., Nicaise C., Usakewicz J., et al. (1993). Phase I trial of chimeric (human-mouse) monoclonal antibody L6 in patients with non-small-cell lung, colon, and breast cancer. Cancer Immunol Immunother.
5 Natarajan A., Gruettner C., Ivkov R., DeNardo G.L., Mirick G., Yuan A., Foreman A., DeNardo S.J. (2008). NanoFerrite particle based radioimmunonanoparticles: binding affinity and in vivo pharmacokinetics. Bioconjug Chem.